# (S)-6-[(4-Chlorophenyl)(1H-1,2,4-triazol-1-yl)methyl]-1-[^11^C]methyl-1H-benzotriazole

Chemical name: | (S)-6-[(4-Chlorophenyl)(1H-1,2,4-triazol-1-yl)methyl]-1-[^11^C]methyl-1H-benzotriazole
Abbreviated name: | [^11^C]Vorozole, [N-methyl-^11^C]Vorozole
Synonym:
Agent category: | Compound
Target: | Aromatase
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole)]

Aromatase is an enzyme complex of the cytochrome P450 superfamily (1). It is composed of P450 and a flavoprotein called NADPH-P450 reductase. Its main function is to aromatize androgens to estrogens. Aromatase is present in many tissues, including granulosa cells of the ovary, brain, fat, placenta, blood vessels, skin, bone, and endometrium. Aromatase is overexpressed in tissue of endometriosis, uterine fibroids, breast cancer, and endometrial cancer (2-6). (S)-6-[(4-Chlorophenyl)(1H-1,2,4-triazol-1-yl)methyl]-1-methyl-1H-benzotriazole (vorozole) is an aromatase inhibitor with a inhibition constant (K_i_) value of 1 nM. Lidstrom et al. (7) prepared [^11^C]vorozole by N-methylation of (S)-6-[(4-chlorophenyl)(1H-1,2,4-triazol-1-yl)methyl]-1H-benzotriazole (nor-vorozole) to use as a positron emission tomography (PET) radioligand to study aromatase activity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20synthesis)]

Lidstrom et al. (7) reported the radiosynthesis of [^11^C]Vorozole by N-methylation of the nor-vorozole using [^11^C]methyl iodide in the presence of KOH. [N-methyl-^11^C]Vorozole was obtained with 53–56% radiochemical yield based on [^11^C]methyl iodide within 40 min of the end of radionuclide production with radiochemical purity of >98% and a specific radioactivity of 10–143 GBq/µmol (0.27–3.86 Ci/µmol). [N-methyl-^11^C]Vorozole (N-1) was the major product of the N-1 methylation reaction and N-3 isomer was formed with N-3 methylation in a ratio of 5:2. Lidstrom et al. (7) and Takahashi et al. (8) used the mixture for imaging studies.

Using the same reaction, Kim et al. (9) found a mixture of N-methylation (N-1, N-2, and N-3) isomers (1:1:1 ratio) using HPLC analysis with a pentafluorophenylpropyl bonded silica column. The radiochemical purity and radiochemical yield of each isomer was >97% and ~30%, respectively. The specific activity was 0.3-0.7 GBq/µmol (10-19 Ci/µmol). Total synthesis time was 65 min after the end of bombardment. The log D_7.4_ lipophilicity values were 2.5, 2.9, and 2.5 for the N-1, N-2, and N-3 isomers, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20in%20vitro)]

Lidstrom et al. (7) performed [^11^C]vorozole autoradiography in frozen sections of human placenta, pig liver, and pig duodenum with 98%, 59%, and 41% specific binding, respectively. The [^11^C]vorozole affinity binding constant (K_d_) to the human placenta aromatase was determined to be 1.7 nM, reaching the binding equilibrium in ~2 min. Kirilovas et al. (10) reported a K_d_ value of 0.44 ± 0.25 nM and a maximum binding (B_max_) of 11.2 ± 7.0 fmol/4,000 cells using [^11^C]vorozole binding to human granulose cells. Takahashi et al. (11) reported that [^11^C]vorozole exhibited a K_d_ value of 0.60 ± 0.06 nM and a B_max_ value of 9.3 ± 1.1 fmol/mg wet tissue using male rat medial amygdale.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Takahashi et al. (8) demonstrated that the androgenic steroid nandrolone decanoate increased aromatase expression in the bed nucleus of stria terminals and preoptic areas in rat brain with [^11^C]vorozole autoradiography. Further studies indicated a significant increase of [^11^C]vorozole binding by nandrolone decanoate in the bed nucleus of the stria terminalis and preoptic area (12). Immunohistochemical examination demonstrated that upregulation of aromatase expression occurred in neurons. Flutamide (anti-androgen) treatment decreased [^11^C]vorozole binding in the bed nucleus of the stria terminalis, preoptic area, and medial amygdala.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%20Terms%5D%20NOT%20%22primates%22%5BMeSH%5D)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20%22primates%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D)]

Lidstrom et al. (7) performed PET imaging to study tissue accumulation of 110–160 MBq (3.0–4.3 mCi) [^11^C]vorozole (N-1 + N-3) in two rhesus monkeys for 60 min after injection. The liver exhibited the highest initial accumulation of 20% injected dose (ID), which declined only slightly by 60 min. After initial accumulation, radioactivity in the brain, kidneys, and lungs decreased to levels <2% ID at 60 min after injection. When a pharmacological dose of vorozole (0.003 mg/kg) was administered 30 min before the tracer, there were only minor changes in the biodistribution of [^11^C]vorozole in the liver, lung, and heart, with moderate inhibition in the brain. On the other hand, Takahashi et al. (11) showed that vorozole (0.1 mg/kg) at a higher dose was able to block [^11^C]vorozole accumulation in the amygdala in the rhesus monkey brain. The fraction of unchanged [^11^C]vorozole in plasma samples as determined with high-performance liquid chromatography was 85% at 10 min, 77% at 20 min, and 68% at 45 min after injection.

Kim et al. (9) performed PET imaging studies with 164 MBq (4.4 mCi) N-1, 45 MBq (1.2 mCi) N-2, 123 MBq (3.3 mCi) N-3 and the mixture (N-1 + N-3) in the baboon brains for 90 min after injection. Time-activity curves for pure [N-methyl-^11^C]vorozole (N-1) in the baboon brain revealed very high initial uptake in five brain regions (the amygdala, cerebellum, frontal cortex, white matter and preoptic area). Radioactivity levels peaked at ~5 min and cleared to a low point at 20–30 min and relatively stable accumulation through the end of the study in the five brain regions. The amygdala and preoptic area exhibited the highest accumulation of radioactivity. Pretreatment with vorozole (0.1 mg/kg) inhibited the N-1 accumulation the five brain regions. On the other hand, no specific binding was observed with N-2, N-3 and the mixture in the amygdala and preoptic area. The amygdala/cerebellum ratios were 1.6, 1.0, and 0.9 for N-1, N-1 + N-3, and N-3, respectively. Therefore, pure N-1 isomer of [N-methyl-^11^C]vorozole should be used for further imaging of aromatase activity in the brain.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Vorozole%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

No publication is currently available.

## NIH Support

K05 DA020001

## References

1 Cole P.A., Robinson C.H. (1990). Mechanism and inhibition of cytochrome P-450 aromatase. J Med Chem.
2 Rojo F., Albanell J., Rovira A., Corominas J.M., Manzarbeitia F. (2008). Targeted therapies in breast cancer. Semin Diagn Pathol.
3 El-Gizawy, Z., E. Tzakas, and P.M. O'Brien, Systematic review of the effects of aromatase inhibitors on pain associated with endometriosis. Bjog, 2008115(13): p. 1721-2; author reply 1722.
4 Bulun S.E., Simpson E.R. (2008). Aromatase expression in women's cancers. Adv Exp Med Biol.
5 Sankaran S., Manyonda I.T. (2008). Medical management of fibroids. Best Pract Res Clin Obstet Gynaecol.
6 Bukulmez O., Hardy D.B., Carr B.R., Word R.A., Mendelson C.R. (2008). Inflammatory status influences aromatase and steroid receptor expression in endometriosis. Endocrinology.
7 Lidstrom P., Bonasera T.A., Kirilovas D., Lindblom B., Lu L., Bergstrom E., Bergstrom M., Westlin J.E., Langstrom B. (1998). Synthesis, in vivo rhesus monkey biodistribution and in vitro evaluation of a 11C-labelled potent aromatase inhibitor: [N-methyl-11C]vorozole. Nucl Med Biol.
8 Takahashi K., Hallberg M., Magnusson K., Nyberg F., Watanabe Y., Langstrom B., Bergstrom M. (2007). Increase in [11C]vorozole binding to aromatase in the hypothalamus in rats treated with anabolic androgenic steroids. Neuroreport.
9 Kim S.W., Biegon A., Katsamanis Z.E., Ehrlich C.W., Hooker J.M., Shea C., Muench L., Xu Y., King P., Carter P., Alexoff D.L., Fowler J.S. (2009). Reinvestigation of the synthesis and evaluation of [N-methyl-(11)C]vorozole, a radiotracer targeting cytochrome P450 aromatase. Nucl Med Biol.
10 Kirilovas D., Naessen T., Bergstrom M., Bonasera T.A., Bergstrom-Pettermann E., Holte J., Carlstrom K., Simberg N., Langstrom B. (2003). Effects of androgens on aromatase activity and 11C-vorozole binding in granulosa cells in vitro. Acta Obstet Gynecol Scand.
11 Takahashi K., Bergstrom M., Frandberg P., Vesstrom E.L., Watanabe Y., Langstrom B. (2006). Imaging of aromatase distribution in rat and rhesus monkey brains with [11C]vorozole. Nucl Med Biol.
12 Takahashi K., Tamura Y., Watanabe Y., Langstrom B., Bergstrom M. (2008). Alteration in [11C]vorozole binding to aromatase in neuronal cells of rat brain induced by anabolic androgenic steroids and flutamide. Neuroreport.